# ^64^Cu-Labeled L-histidine

Chemical name: | ^64^Cu-Labeled L-histidine
Abbreviated name: | [^64^Cu]-His
Synonym:
Agent Category: | Compound
Target: | Copper transporter I (Ctr1)
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Wilsons%20disease&cmd=DetailsSearch)]

Copper (Cu) metal is not commonly available in the environment, but is an important micronutrient that is required for the activity of many mammalian intracellular enzymes (1). Presence of free Cu is toxic for the cell because it can exist in the oxidized (Cu(I)) or the reduced (Cu(II)) forms, and conversion of Cu(I) to Cu(II) under physiological conditions leads to the generation of reactive oxygen species that disrupt the normal cellular pathways. Therefore, mammals tend to maintain extremely low concentrations of the metal within tissues, which is achieved by transporting it out of the cells into the circulatory system and eventually into the bile for excretion through the hepatobiliary system (2). In the liver, the Cu transporter 1 helps in the passage of the metal into the hepatocytes, and the ATP7B gene product, a Cu-transporting polypeptide (for details, see the Related Resource Links section), is responsible for removing Cu from the liver cells for excretion into the bile. However, genetic mutations in ATP7B result in impaired excretion and intracellular utilization of the metal in mammals. This culminates in accumulation of toxic amounts of Cu in various organs, particularly the liver and the brain, and leads to the development of Wilson disease (http://digestive.niddk.nih.gov/ddiseases/pubs/wilson/) (WD) in humans (3).

Although treatment is available for the therapy of WD, it is challenging to diagnose the disease because there are many variations in the symptoms of this condition (2, 3). Currently WD is diagnosed only after a liver biopsy; the Cu content of the hepatic tissues can be best determined with atomic force spectroscopy, a technique that is not commonly available in the clinic (4). The unsuccessful use of ^64^Cu for the diagnosis of WD has been attributed to the wide distribution of the element in the body and to the constant release and reuptake of the metal by different organs in the body (4). Bahde et al. hypothesized that, because the Cu excretion process is ATP7B-dependent, the use of ^64^Cu complexed with histidine ([^64^Cu]-His) was probably suitable for the diagnosis of WD because it was shown that [^64^Cu]-His can be utilized to determine the ^64^Cu biliary excretion capacity in animals (4). The biodistribution of [^64^Cu]-His was investigated in Long-Evans cinnamon (LEC) rats, which have a mutated ATP7B and show a very high accumulation of Cu in the liver, and this biodistribution was compared with the biodistribution in Long-Evans agouti (LEA) rats that have a normally functioning ATP7B. In addition, dynamic positron emission tomography (PET) imaging was performed on the animals to visualize the excretion of ^64^Cu from the liver of these animals.

### Related Resource Links

Wilson disease (http://www.genome.jp/dbget-bin/www_bget?ds:H00210) in Kyoto Encyclopedia of Genes and Genomes (KEGG)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Wilsons+disease) regarding Wilson disease

Copper histidine (http://clinicaltrials.gov/ct2/results?term=Copper+histidine) related clinical trials

Drug to treat Wilson disease (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=38f8ae60-b354-11de-8a39-0800200c9a66)

Copper transporter 1 (http://omim.org/entry/603085) in Online Mendelian Inheritance in Man Database (OMIM)

ATP7B gene product (http://omim.org/entry/606882) in OMIM

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20synthesis&cmd=DetailsSearch)]

L-Histidine was obtained from a commercial source and labeled with ^64^Cu as described by Bahde et al. (4). The labeled product was purified on a SepPak C_18_ cartridge and eluted in water. The radiochemical purity and the radiochemical yield of the purified [^64^Cu]-His were >95% (as determined with instant thin-layer chromatography) and 91% (based on the amount of ^64^Cu added to the reaction mixture), respectively. The specific activity of [^64^Cu]-His was 700–750 MBq (19.9–20.25 mCi)/4.54 μmol. The stability of the final product was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20In%20Vitro%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20rodentia&cmd=DetailsSearch)]

On the basis of ATP7B mRNA expression in the rodents, the three genotypes of rats (n = 6 animals/genotype) used in the animal studies were as follows: the LEA (+/+) rats expressed the ATP7B mRNA normally, the LEC (–/–) rats were homozygous and completely lacked expression of the ATP7B mRNA (4), and the LEC (+/–) rats were heterozygous for expression of the mRNA because these animals had normal hepatocytes transplanted from donor LEA (+/+) rats (4). The livers and hepatocytes of the LEA (+/+) and the LEC (+/–) rats were reported to have a normal morphology, but in the LEC (–/–) rats the hepatocytes were enlarged, and the organ showed biliary proliferation and fibrosis. The Cu contents of the liver from LEA (+/+), LEC (+/–), and the LEC (–/–) rats were 20 ± 13 μg/g, 44 ± 38 μg/g, and 860 ± 58 μg/g, respectively, indicating that the LEC (–/–) animals accumulated high levels of Cu in the organ.

To investigate the biodistribution of radioactivity from [^64^Cu]-His in the different genotypes of rats (n = 9 animals/genotype), the rodents were injected with 3.7–5.5 MBq (100–150 μCi) of the tracer through the intrasplenic route (4). Bile and the organs of interest were collected from the rodents at various time points, ranging from 0 min to 24 h post-injection (p.i.), to determine the amount of accumulated radioactivity in the bile and the different tissues. All results were presented as percent of total injected dose per gram tissue (% ID/g). The rate of radioactivity clearance from the blood was rapid, medium, and very slow in the LEC (–/–), LEC (+/–), and LEA (+/+) rats, respectively (Table 1). In general, the accumulation of radioactivity was highest in the liver, followed by the kidney and the spleen for all the rat genotypes. As expected, the liver of LEC (–/–) rats had a significantly higher (P < 0.05) amount of label compared with the organs from either the LEA (+/+) or the LEC (+/–) animals. The excretion of label into the bile of the different animals was studied for up to 24 h p.i. as described by Bahde et al. (4). Both the LEA (+/+) and the LEC (+/–) animals showed a gradual and comparable secretion of radioactivity into the bile during this period; however, the LEC (–/–) animals showed no secretion of label into the bile for the entire duration of the study and showed a significantly increased accumulation (P < 0.05) of the tracer up to 24 h p.i. This indicated that the biliary excretion of radioactivity in the LEA (+/+) and the LEC (+/–) rats was due to the presence of an active ATP7B gene.

Table 1: Amount of radioactivity (% ID/g) in blood ( 4 ).

Genotype | Blood | | Rate of clearance
Genotype | Time p.i. | | Rate of clearance
Genotype | 45 min | 24 h | Rate of clearance
LEA (+/+) | 74 ± 5 | 71 ± 9 | Very low
LEC (+/–) | 75 ± 5 | 50 ± 12* | Medium
LEC (–/–) | 61 ± 5 | 9 ± 2* | Rapid

*P < 0.05 compared to the amount of label at 45 min p.i.

For PET imaging, anesthetized rats were injected with 18.5 MBq (500 μCi) [^64^Cu]-His as before, and dynamic images of the animals (n = 3 rats/genotype per time point) were acquired at 1 h, 3 h, and 24 h p.i. as described elsewhere (4). From the images it was clear that the level of radioactivity accumulated in livers of the LEA (+/+) and LEC (+/–) rats at 1 h p.i. had decreased by 3 h p.i. and was further reduced by 24 h p.i. The loss of radioactivity from the liver was consistent with the appearance of the tracer in the bile of these animals during the same period. In the LEC (–/–), rats the amount of label in the liver gradually increased from 1 h p.i. to 24 h p.i., indicating that there was little to no loss of ^64^Cu from this organ in these animals for up to 24 h p.i.

In a separate study, it was shown that acute liver injuries in normal LAE (+/+) rats (n = 6 animals) or chronic liver injuries in normal F344 rats (n = 9 animals) did not alter the uptake and excretion of ^64^Cu in the liver of these rodents (4). Similar observations were made when LAE (+/+) rats were treated with drugs that increased the flow of bile (sodium valproate or hydrocortisone) in these animals (4). In another study, it was observed that the clearance of ^64^Cu from the blood of rats (number of animals not mentioned) with cirrhotic livers (induced with repeated carbon tetrachloride treatment) was slower than that in healthy rats, and the amount of label present in the diseased liver was lower compared to that in the hepatic tissue of the LEC (–/–) animals (4).

From these studies, the investigators concluded that [^64^Cu]-His can be used with PET imaging to detect WD in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu-histidine%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported in part by National Institutes of Health grants R01DK088561, R01DK071111, and P30DK41296.

## References

1 Tsigelny I.F., Sharikov Y., Greenberg J.P., Miller M.A., Kouznetsova V.L., Larson C.A., Howell S.B. (2012). An all-atom model of the structure of human copper transporter 1. Cell Biochem Biophys.
2 Weiss K.H., Stremmel W. (2012). Evolving perspectives in Wilson disease: diagnosis, treatment and monitoring. Curr Gastroenterol Rep.
3 Bennett J., Hahn S.H. (2011). Clinical molecular diagnosis of Wilson disease. Semin Liver Dis.
4 Bahde R., Kapoor S., Bhargava K.K., Schilsky M.L., Palestro C.J., Gupta S. (2012). PET with 64Cu-Histidine for Noninvasive Diagnosis of Biliary Copper Excretion in Long-Evans Cinnamon Rat Model of Wilson Disease. J Nucl Med.